# 3-(Pyridin-2-ylethynyl)-cyclohex-2-enone-O-[^18^F]fluoroethyl-oxime

Chemical name: | 3-(Pyridin-2-ylethynyl)-cyclohex-2-enone-O-[^18^F]fluoroethyl-oxime
Abbreviated name: | [^18^F]FE-DABP688
Synonym: | [^18^F]Fluoroethyl-desmethyl-ABP688
Agent Category: | Compound
Target: | Metabotropic glutamate receptor subtype 5 (mGluR5)
Target Category: | Receptor-ligand binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FE-DABP688)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). Many neuronal projection pathways contain mGluRs. The mGluRs are GTP-binding-protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS. There are eight mGluR subtypes. The fifth subtype, mGluR5, is usually found in postsynaptic neurons with moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. The mGluR5 is positively coupled to phospholipase C in regulation of neuronal excitability (2). Dysfunction of mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (3).

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting mGluR5 can visualize and analyze mGluR5 in normal physiological and pathological conditions. 2-Methyl-6-(phenylethynyl)-pyridine (MPEP) and its methyl analog M-MPEP have been identified as potent and highly selective noncompetitive antagonists for mGluR5. These mGluR5 antagonists have been successfully labeled, but their impact as targeted imaging agents has been limited by high lipophilicity, lack of mGluR subtype selectivity, and unfavorable brain accumulation kinetics (4, 5). Based on the structure of MPEP, 3-(6-methyl-pyridin-2-ylethynyl)-cyclohex-2-enone-O-[^11^C]-methyl-oxime ([^11^C]ABP688) was synthesized and evaluated as a potential PET imaging agent for mGluR5, showing strong and specific signals in the rodent and human brain (6-9). Using ABP688 as a template, 3-(pyridin-2-ylethynyl)-cyclohex-2-enone-O-[^18^F]fluoroethyl-oxime ([^18^F]fluoroethyl-desmethyl-ABP688 or [^18^F]FE-DABP688) was synthesized and evaluated as a specific PET imaging tool for mGluR5 (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-DABP688%20and%20synthesis)]

Honer et al. (10) reported a two-step synthesis of [^18^F]FE-DABP688. First, [^18^F]fluoroethyl-tosylate was synthesized by nucleophilic fluorination of ethyleneglycol-1,2-ditosylate with K[^18^F]F/Kryptofix 2.2.2 at 85°C for 10 min. Second, 3-(pyridin-2-ylethynyl)-cyclohex-2-enone-oxime reacted with [^18^F]fluoroethyl-tosylate via alkylation at 100°C for 10 min with an average yield of 25 ± 8% (decay-corrected) and a specific activity of 30 ± 5 GBq/μmol (0.81 ± 0.14 Ci/μmol) after purification with high-performance liquid chromatography. The total synthesis time was 150 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-DABP688%20and%20in%20vitro)]

The distribution coefficient (log D, pH 7.4) of [^18^F]FE-DABP688, as determined by Honer et al. (10), was 2.1 ± 0.1 (n = 7). [^18^F]FE-DABP688 was stable in human blood and in vitro plasma at 37°C for up to 120 min. In vitro binding of [^18^F]FE-DABP688 was studied in rat brain tissue membranes. Saturation studies indicated that the receptor binding was saturable, and the Scatchard plot analysis indicated a single high-affinity binding site with a dissociation constant of 1.4 ± 0.4 nM (n = 3) and a maximal binding of 119 ± 24 fmol/mg protein.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-DABP688%20and%20rodentia)]

Honer et al. (10) performed in vivo biodistribution studies in normal rats that received intravenous injections of 15 MBq (0.41 mCi, 0.5 nmol) [^18^F]FE-DABP688. Results showed that the highest radioactivity concentrations (expressed as injected dose/gram (ID/g)) were observed in mGluR5-rich brain regions such as the hippocampus (0.40% ID/g) and striatum (0.44% ID/g), whereas radioactivity accumulation was lowest in the cerebellum (0.22% ID/g) at 20 min after injection (the only time point studied). The hippocampus/cerebellum and striatum/cerebellum ratios were 1.81 ± 0.16 and 1.93 ± 0.36, respectively. Co-injection of 1 mg/kg M-MPEP, a specific ligand for mGluR5, with [^18^F]FE-DABP688 decreased the accumulation of radioactivity by 50% in the hippocampus and striatum, whereas no significant inhibition was observed in the cerebellum. The peripheral organ with the highest accumulation was the kidney (0.55% ID/g), followed by the liver, bone, lung, blood, and muscle with radioactivity levels of 0.20–0.35% ID/g. PET imaging confirmed highest radioactivity levels in the kidneys and liver. The hippocampus and lacrimal glands were visualized.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-DABP688%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-DABP688%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-DABP688%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
3 Pin J.P., De Colle C., Bessis A.S., Acher F. (1999). New perspectives for the development of selective metabotropic glutamate receptor ligands. Eur J Pharmacol.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Yu M., Tueckmantel W., Wang X., Zhu A., Kozikowski A.P., Brownell A.L. (2005). Methoxyphenylethynyl, methoxypyridylethynyl and phenylethynyl derivatives of pyridine: synthesis, radiolabeling and evaluation of new PET ligands for metabotropic glutamate subtype 5 receptors. Nucl Med Biol.
6 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and preclinical evaluation of 11C-ABP688 as a probe for imaging the metabotropic glutamate receptor subtype 5. J Nucl Med.
7 Ametamey S.M., Treyer V., Streffer J., Wyss M.T., Schmidt M., Blagoev M., Hintermann S., Auberson Y., Gasparini F., Fischer U.C., Buck A. (2007). Human PET studies of metabotropic glutamate receptor subtype 5 with 11C-ABP688. J Nucl Med.
8 Hintermann S., Vranesic I., Allgeier H., Brulisauer A., Hoyer D., Lemaire M., Moenius T., Urwyler S., Whitebread S., Gasparini F., Auberson Y.P. (2007). ABP688, a novel selective and high affinity ligand for the labeling of mGlu5 receptors: identification, in vitro pharmacology, pharmacokinetic and biodistribution studies. Bioorg Med Chem.
9 Wyss M.T., Ametamey S.M., Treyer V., Bettio A., Blagoev M., Kessler L.J., Burger C., Weber B., Schmidt M., Gasparini F., Buck A. (2007). Quantitative evaluation of 11C-ABP688 as PET ligand for the measurement of the metabotropic glutamate receptor subtype 5 using autoradiographic studies and a beta-scintillator. Neuroimage.
10 Honer M., Stoffel A., Kessler L.J., Schubiger P.A., Ametamey S.M. (2007). Radiolabeling and in vitro and in vivo evaluation of [(18)F]-FE-DABP688 as a PET radioligand for the metabotropic glutamate receptor subtype 5. Nucl Med Biol.